# ^125^I-Labeled monoclonal antibody, mAb RM2, targeting the RM2 antigen

Chemical name: | ^125^I-Labeled monoclonal antibody, mAb RM2, targeting the RM2 antigen
Abbreviated name: | [^125^I]-mAb RM2
Synonym:
Agent Category: | Antibody
Target: | RM2 antigen
Target Category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=RM2&cmd=DetailsSearch)]

A prostate-specific antigen (PSA) level of >4 ng/mL in the serum is considered to indicate the development of prostate cancer (http://www.mayoclinic.com/health/prostate-cancer/DS00043) in men; however, PSA levels may be elevated in an individual due to benign prostatic hyperplasia (http://www.mayoclinic.com/health/prostate-gland-enlargement/DS00027) or prostatitis (http://www.mayoclinic.com/health/prostatitis/DS00341) (1). In addition, PSA is an organ-specific biomarker, not a cancer-specific biomarker, which means that the serum PSA level cannot be used to determine the stage of the cancer (2). Therefore, the occurrence of prostate cancer in men with high PSA levels has to be confirmed with an invasive and painful biopsy (2). In an effort to develop a more reliable diagnostic test for prostate cancer, a monoclonal antibody (mAb) that recognizes a disialoganglioside (β1,4-GalNAc-disialyl-Lc4; designated as the RM2 antigen (mAb RM2)) was developed. mAb RM2 was shown to have a high reactivity toward malignant prostate cancer cells, but it exhibited little or no binding to cells obtained from the benign glands (1). It was also shown that the RM2 antigen was overexpressed on prostate cancer cells, and the increased level of the antigen detected in the serum of prostate cancer patients correlated with the Gleason grading (http://cancer.gov/dictionary?cdrid=45696) of the neoplasm. From this study, the investigators concluded that the RM2 antigen may be suitable for the detection of prostate cancer.

Early detection and treatment of cancer is often beneficial for the patient, but prostate cancer is not easily diagnosed during the early stages because imaging techniques that are used to detect this cancer, such as ultrasound, magnetic resonance imaging, and computed tomography, do not yield reliable results (3). Therefore, mAb RM2 was radioiodinated ([^125^I]-mAb RM2) in an attempt to produce a tracer that could be used to detect prostate cancer (3). In a preliminary study, the biodistribution of [^125^I]-mAb RM2 was investigated in athymic nu/nu mice bearing PC-3 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1435&Template=cellBiology) cell tumors (a human prostate adenocarcinoma cell line that overexpresses the RM2 antigen).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-mAb%20RM2%20synthesis&cmd=DetailsSearch)]

mAb RM2 was produced as described elsewhere (1). The mAb was labeled with ^125^I using the chloramine-T method, and the specific activity of [^125^I]-mAb RM2 was reported to be 376 MBq/6.66 nmol (13.9 mCi/6.66 nmol). The radiochemical yield, radiochemical purity, and stability of the labeled mAb were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-mAb%20RM2%20in%20vitro%20studies&cmd=DetailsSearch)]

The uptake of [^125^I]-mAb RM2 by PC-3 cells (an androgen-dependent cell line), LNCaP cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1740&Template=cellBiology) (a human prostate carcinoma cell line that overexpresses the RM2 antigen; an androgen-independent cell line), and MCF-7 cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-22&Template=cellBiology) (a human mammary gland adenocarcinoma cell line that does not express the RM2 antigen) was investigated (3). The cells were incubated with 3.7 kBq (0.1 μCi) [^125^I]-mAb RM2 without or after a 48-h exposure to nonradiolabeled mAb RM2 (concentration not reported) for various time points ranging from 1 h to 6 h. Radioactivity taken up by the different cells was reported as percent uptake of added dose (% AD). The amount of radioactivity taken up by the PC-3 cells increased from 0.045 ± 0.011% AD at 1 h to 0.061 ± 0.005% AD at 6 h (P < 0.05); for the LNCaP cells, the accumulation increased from 0.029 ± 0.005% AD at 1 h to 0.040 ± 0.006% AD at 6 h (P < 0.05). When the PC-3 cells and the LNCaP cells were pre-exposed to nonradioactive mAb RM2, no increase in uptake of the probe was observed. The MCF-7 cells showed no increase in the incorporation of radioactivity from 1 h to 6 h with or without exposure to nonradioactive mAb RM2. This study indicated that mAb RM2 had a binding specificity for the transformed prostate cell lines that overexpress the RM2 antigen.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-mAb%20RM2%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^125^I]-mAb RM2 was studied in athymic nu/nu male mice bearing PC-3 cell tumors (3). The animals (n = 5 mice/time point) were injected with ~0.3 MBq (10 μCi) [^125^I]-mAb RM2 through the tail vein and euthanized at 24, 48, and 72 h postinjection (p.i.) to harvest the organs of interest and to determine the amount of radioactivity taken up by the various tissues. Data obtained from this study were expressed as percent of radioactivity of injected dose per gram tissue (% ID/g).

Table 1: Uptake of radioactivity from [ ^ 125 ^ I]-mAb RM2 by various organs of mice ( 3 ).

Tissue | Time points (h) postinjection
Tissue | 24 | 48 | 72
Tissue | Accumulated radioactivity (% ID/g)*
Blood | 2.88 ± 0.63 | 0.93 ± 0.16 | 0.50 ± 0.08
Liver | 4.32 ± 0.90 | 3.00 ± 0.49 | 2.23 ± 0.28
Muscle | 0.21 ± 0.07 | 0.08 ± 0.02 | 0.05 ± 0.01
Prostate | 0.48 ± 0.21 | 0.19 ± 0.10 | 0.15 ± 0.02
Tumor | 0.40 ± 0.03 | 0.27 ± 0.10 | 0.17 ± 0.02
Tumor/muscle ratio# | 2.12 ± 0.88 | 3.13 ± 0.67 | 3.47 ± 0.78

* For complete data, see Hasegawa et al. ( 3 ); #: P < 0.05 for 24 h versus 72 h.

The uptake of radioactivity from [^125^I]-mAb RM2 by select organs, including tumors, is presented in Table 1. At 24 h p.i., maximum uptake of label was in the liver followed by blood. Although both tissues showed loss of radioactivity from 24 h p.i. to 72 h p.i., the decrease in the blood was faster than that in the liver, suggesting that the probe was excreted from the body through the hepatobiliary system. The tumor/muscle (T/M) ratio was reported to significantly increase (P < 0.05) from 24 h p.i. (2.12 ± 0.88) to 72 h p.i. (3.47 ± 0.78). The insignificant difference in the uptake of radioactivity between the normal prostate tissue and the PC-3 cell tumors in the mice was attributed to the differences between the human and mouse species (the PC-3 cells used to generate tumors in the rodents were of human origin) (3).

From these preclinical studies, the investigators concluded that the radiolabeled mAb RM2 could probably be used in conjunction with the PSA test to diagnose prostate cancer (3). They also suggested that mAb RM2 may be used by itself to distinguish between malignant and benign tumors in the prostate gland.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-mAb%20RM2%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-mAb%20RM2%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-mAb%20RM2%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Saito S., Egawa S., Endoh M., Ueno S., Ito A., Numahata K., Satoh M., Kuwao S., Baba S., Hakomori S., Arai Y. (2005). RM2 antigen (beta1,4-GalNAc-disialyl-Lc4) as a new marker for prostate cancer. Int J Cancer.
2 Saito S., Murayama Y., Pan Y., Taima T., Fujimura T., Murayama K., Sadilek M., Egawa S., Ueno S., Ito A., Ishidoya S., Nakagawa H., Kato M., Satoh M., Endoh M., Arai Y. (2008). Haptoglobin-beta chain defined by monoclonal antibody RM2 as a novel serum marker for prostate cancer. Int J Cancer.
3 Hasegawa Y., Oyama N., Nagase K., Fujibayashi Y., Furukawa T., Murayama Y., Arai Y., Saito S., Welch M.J., Yokoyama O. (2012). Monoclonal antibody RM2 as a potential ligand for a new immunotracer for prostate cancer imaging. Nucl Med Biol.